# ^64^Cu-Labeled bis-1,4,7,10-tetraazacyclododecane-N,N',N,N'-tetraacetic acid conjugated hypericin

Chemical name: | ^64^Cu-Labeled bis-1,4,7,10-tetraazacyclododecane-N,N',N,N'-tetraacetic acid conjugated hypericin
Abbreviated name: | [^64^Cu]-bis DOTA-hypericin
Synonym:
Agent Category: | Compound
Target: | Tumor necrosis (cell membranes and subcellular organelle membranes)
Target Category: | Other
Method of detection: | Positron emission tomography (PET)
Source of signal / contrast: | ^64^Cu
Activation: | No
Studies: | - In vitro; - Rodents | Click on the above structure of Hypericin for additional information in PubChem (http://pubchem.ncbi.nlm.nih.gov/).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=hypericin&cmd=DetailsSearch)]

A common problem encountered with the chemotherapy or radiotherapy of cancer is the development of resistance to these treatments resulting in metastasis of the malignancy. Therefore, there is an urgent need to develop new anti-cancer treatments that have a unique mechanism of action and are not prone to the development of drug or radiation resistance (1). Photothermal ablation (PTA) therapy is an emerging technique that uses heat produced from absorbed light to destroy cancer cells. PTA therapy can be performed frequently, has no side effects, and does not promote the development of resistance (1). For PTA therapy, near-infrared (NIR) light is used to deliver a predetermined amount of photothermal energy directly into a tumor, which stimulates photochemical and photothermal reactions within the malignant lesion that are fatal for the cancer cells (2). In addition, the application of PTA in the presence of a light-absorbing nanoparticles (NPs), such as gold NPs (shells, rods, and cages) or copper sulfide (CuS) NPs, has been shown to enhance efficacy of the therapy (3). However, many parameters, such as the dose of NIR required to maximize the efficacy of PTA therapy, the number of NPs required for optimal ablation, or how to monitor the treatment noninvasively, remain to be worked out (1).

Computed tomography, magnetic resonance imaging, and ultrasonography are currently used to monitor morphological changes that occur after PTA therapy, but alterations in the tissue are visible with these techniques for only 2–3 months after initiation of the treatment (1). It is well known that ^18^F-labeled fluorodeoxyglucose ([^18^F]-FDG) is often used with positron emission tomography (PET) to assess the response to cancer therapy, but this imaging modality generates reliable results for only 2–3 weeks after initiation of the treatment. In addition, [^18^F]-FDG can generate false-positive results because it also detects inflammation (http://dictionary.webmd.com/terms/inflammation), sarcoidosis (http://www.lungusa.org/lung-disease/sarcoidosis/?gclid=CIapzbbzzqgCFUOo4AodlSW-gA), and fungal (http://www.merckmanuals.com/home/sec17/ch197/ch197a.html) and tuberculosis (http://www.webmd.com/lung/tc/tuberculosis-tb-topic-overview) infections (lesions from these conditions show an upregulated glucose metabolism similar to that of cancer cells) (1, 4). Hypericin, a naturally occurring polycyclic quinone that can be isolated from the plant Hypericum perforatum (http://plants.usda.gov/java/profile?symbol=HYPE) or chemically synthesized, has been investigated for the photodynamic therapy of cancer and other conditions (5). Although the exact mechanism of action of this compound is not known, several reports suggest that multiple cellular pathways participating in the survival, necrosis (http://dictionary.webmd.com/terms/necrosis), or apoptosis (http://dictionary.webmd.com/terms/apoptosis) of the cell are involved in bringing about the activity of hypericin as discussed elsewhere (5, 6). Hypericin is considered a nonporphyrin agent that binds to necrotic tissues, and ^123^I-labeled hypericin has been shown to detect tissue necrosis in the liver and the heart [PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=123I-hypericin)]. Song et al. synthesized ^64^Cu-labeled bis-1,4,7,10-tetraazacyclododecane-N,N',N,N'-tetraacetic acid (DOTA)-conjugated hypericin ([^64^Cu]-bis-DOTA-hypericin) and used it to evaluate the response of xenograft human BT474 breast carcinoma cell (http://www.atcc.org/ATCCAdvancedCatalogSearch/ProductDetails/tabid/452/Default.aspx?ATCCNum=HTB-20&Template=cellBiology) tumors in nude mice subjected to PTA treatment in presence of copper sulfide nanoparticles (CuS NPs) (1). The biodistribution of [^64^Cu]-bis-DOTA-hypericin was also investigated in these animals.

### Other Sources of Information

Related chapters in MICAD (http://www.ncbi.nlm.nih.gov/books/?term=Hypericin+AND+micad%5Bbook%5D&view=chapter&p%24a=&p%24l=PBooksLayout&p%24st=books)

Clinical trials (http://clinicaltrials.gov/ct2/results?term=Hypericin) with hypericin

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/gene?term=64Cu-bis-DOTA-Hypericin%20synthesis&cmd=DetailsSearch)]

The synthesis of [^64^Cu]-bis-DOTA-hypericin has been described by Song et al. (1). The radiochemical yield and purity were reported to be 97.7% and >95%, respectively, as determined with radio-high-performance liquid chromatography. The stability and specific activity of the final product were not reported.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=64Cu-bis-DOTA-hypericin&cmd=DetailsSearch)]

A higher number of BT474 cells died when they were exposed to CuS NPs and treated with a NIR laser compared to cells exposed to either the CuS NP alone or the laser alone (1). The PTA-treated cells were reported to have damaged membranes as observed with uptake studies of ethidium homodimer (http://www.moleculardevices.com/Documents/general-documents/mkt-appnotes/microplate-appnotes/Maxline_AppNote_43 LIVEDEAD.pdf), a red fluorescent dye impermeable to living cells.

In another study, BT474 cells exposed to CuS NPs and treated with a NIR laser showed a significantly higher (P = 0.04) uptake of [^64^Cu]-bis-DOTA-hypericin compared to cells exposed to the CuS NPs or the NIR laser alone (1). Cell exposed to the CuS NPs and the NIR laser were reported to have a much higher uptake of the red, cell-impermeable EthD-1 dye compared to cells treated with the CuS or the NIR laser alone. This suggested the thermal ablation treatment was more effective (i.e. there was an increased cell death) in presence of the CuS NPs and the CuS NPs or the NIR alone had little effect on the cells. To determine the binding specificity of [^64^Cu]-bis-DOTA-hypericin, cells were treated with CuS NPs and NIR laser and exposed to [^64^Cu]-bis-DOTA-hypericin in the presence of excess non-radioactive hypericin. Binding of the labeled compound to these cells was reduced by 54% (P = 0.007) compared to the binding of cells exposed only to [^64^Cu]-bis-DOTA-hypericin (1). This strongly indicated that the labeled hypericin targeted the same cell membrane components as the native hypericin.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=64Cu-bis-DOTA-hypericin%20rodentia&cmd=DetailsSearch)]

The biodistribution of [^64^Cu]-bis-DOTA-hypericin was investigated in nude mice (n = 4–5 animals/time point) bearing BT474 cell tumors as described by Song et al. (1). Animals in the treated group (TG) received an intratumoral injection of CuS NPs (10 μL, 4 × 10^13^ NP/mL) and were irradiated with NIR laser 24 h later (808 nm, 12 W/cm^2^ for 3 min). Control animals (non-targeted (N-TG)) were not injected with the NPs or irradiated with the NIR laser. Both groups of mice were injected with [^64^Cu]-bis-DOTA-hypericin (5.55–7.4 MBq/0.1 mL (150–200 µCi/0.1 mL)) through the tail vein. Small-animal PET scans were subsequently performed on the mice at 2, 6, and 24 h postinjection (p.i.) while the animals were under anesthesia. After the last scan, the mice were euthanized, and major organs (including tumors) were harvested from the animals to determine the amount of radioactivity accumulated in the various tissues. Data were presented as percent of injected dose per gram tissue (% ID/g).

Small-animal PET scans of the animals revealed that tumors on the TG mice were clearly visible from 2 h to 24 h p.i., and tumors on the N-TG mice showed little accumulation of the tracer (1). From quantitative imaging analysis, the amount of radioactivity in tumors of the TG group was reported to be 0.80 ± 0.14% ID/g (P = 0.024), 1.19 ± 0.45% ID/g (P = 0.019), and 1.49 ± 0.68% ID/g (P = 0.039), at 2, 6, and 24 h p.i., respectively, compared to 0.57 ± 0.06% ID/g, 0.50 ± 0.63% ID/g, and 0.53 ± 0.18% ID/g at the same time points for animals in the N-TG group.

Biodistribution data from this study showed that the tumors of the TG and N-TG groups were the only tissues to show a significant difference in the accumulation of radioactivity (1). The uptake of label in tumors of the TG mice (1.71 ± 0.43% ID/g) was significantly higher (P = 0.017) than that observed in tumors of the N-TG mice (0.76 ± 0.19% ID/g). Tissue necrosis and the presence of radioactivity at the tumor site were confirmed with hematoxylin and eosin staining and autoradiography of tumor sections, respectively, as described by Song et al. (1). All other organs from the animals in both groups showed a comparable uptake of the tracer. This suggests that radioactivity derived from [^64^Cu]-bis-DOTA-hypericin had a binding specificity for necrotic tissue developed in the tumors after the PTA treatment. No blocking studies were reported.

On the basis of results obtained from this study, the investigators concluded that [^64^Cu]-bis-DOTA-hypericin can be used for the noninvasive assessment of tumor response to CuS NP-mediated PTA in mice.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=64Cu-bis-DOTA-hypericin%20Non-Primate%20Mammals&cmd=DetailsSearch)]

No publications are currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=64Cu-bis-DOTA-hypericin%20Non-Human%20Primates&cmd=DetailsSearch)]

No publications are currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=64Cu-bis-DOTA-hypericin%20Human%20Studies&cmd=DetailsSearch)]

No publications are currently available.

## Supplemental Information

[Disclaimers]

No information is currently available.

## References

1 Song, S., C. Xiong, M. Zhou, W. Lu, Q. Huang, G. Ku, J. Zhao, L.G. Flores, Jr., Y. Ni, and C. Li, Small-Animal PET of Tumor Damage Induced by Photothermal Ablation with 64Cu-Bis-DOTA-Hypericin. J Nucl Med, 2011
2 Vogel A., Venugopalan V. (2003). Mechanisms of pulsed laser ablation of biological tissues. Chem Rev.
3 Zhou M., Zhang R., Huang M., Lu W., Song S., Melancon M.P., Tian M., Liang D., Li C. (2010). A Chelator-Free Multifunctional [64Cu]CuS Nanoparticle Platform for Simultaneous Micro-PET/CT Imaging and Photothermal Ablation Therapy. Journal of the American Chemical Society.
4 Culverwell A.D., Scarsbrook A.F., Chowdhury F.U. (2011). False-positive uptake on 2-[(1)F]-fluoro-2-deoxy-D-glucose (FDG) positron-emission tomography/computed tomography (PET/CT) in oncological imaging. Clin Radiol.
5 Karioti A., Bilia A.R. (2010). Hypericins as potential leads for new therapeutics. Int J Mol Sci.
6 Theodossiou T.A., Hothersall J.S., De Witte P.A., Pantos A., Agostinis P. (2009). The multifaceted photocytotoxic profile of hypericin. Mol Pharm.